# ^111^Indium-diethylenetriaminepentaacetic acid-D-phenylalanine-octreotide

Chemical name: | ^111^Indium-diethylenetriaminepentaacetic acid-D-phenylalanine-octreotide
Abbreviated name: | ^111^In-DTPA-octreotide; ^111^In-DTPA-OC; ^111^In-DTPA-D-Phe-octreotide;^111^In-pentetreotide
Synonym: | OctreoScan® (commonly used brand name)
Agent Category: | Compound
Target: | Somatostatin receptor (SSR)
Target Category: | Ligand binding to SSR subtypes 2 and 5; subtype 3 to a lesser degree
Method of detection: | SPECT, scintigraphy (planar)
Source of signal: | ^111^In
Activation: | No
Studies: | - In vitro; - Rodents; - Other non-primate mammals; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SDZ%20215-811%22%5BSubstance%20Name%5D)]

Somatostatin (SS) is a tetradecapeptide acting as an inhibitor of the release of somatotropin, glucagon, gastrointestinal hormones, and other secretory proteins. Critical to these actions is the expression of SS receptors (SSRs) present on cell membranes. Such receptors recognize and bind to the ligand with high affinity and specificity and generate a transmembrane signal that induces a biological response. SSRs have been found on a variety of neuroendocrine tumors and cells of the immune system, and five individual subtypes have been identified and subsequently cloned from animal and human tissues (1, 2).

^111^In-DTPA-OC is a SSR analog that, over the last decade, has remained the most widely used radiopharmaceutical for the scintigraphic detection and staging of primary and metastatic neuroendocrine tumors bearing SSRs (mainly growth hormone-secreting pituitary tumors, endocrine pancreatic tumors, carcinoids, brain tumors, and other neuroendocrine tumors with typical amine precursor uptake and decarboxylation characteristics). It has also showed promising results in peptide-receptor radionuclide therapy (3-7). ^111^In-DTPA-OC binds with high affinity to SSR subtypes 2 and 5 (sst_2_ and sst_5_) and to sst_3_ to a lesser degree but does not bind to sst_1_ and sst_4_ (3, 8).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SDZ%20215-811%22%5BSubstance%20Name%5D%20AND%20synthesis%5BAll%20Fields%5D)]

^111^In-DTPA-OC can be easily prepared from a commercially available kit (OctreoScan, Mallinckrodt Medical B.V., Petten, The Netherlands) consisting of two components to be mixed: 1) a sterile solution of 111 MBq/ml (3.0 mCi/ml) ^111^In-choride in 0.02 N HCl with ferric chloride (3.5 µg/ml); and 2) a mixture of 10 µg of pentetreotide (DTPA-octreotide), 2.0 mg gentisic acid, 4.9 mg trisodium citrate, anhydrous, 0.37 mg citric acid, anhydrous, and 10.0 mg of inositol.

^111^In-DTPA-OC can be synthesized and radiolabeled using the protocol described by Bakker et al. (9). One essential step of this method involves coupling DTPA to the protected OC in form of its anhydride (10). Radiolabeling of DTPA-OC with ^111^In is done with a 40-70-molar excess of peptide over the radionuclide (2 µg of peptide in 20 µl of 0.1 M acetic acid with 37 MBq (1 mCi) of ^111^In in 20 µl of 0.04 M HCl). The resulting specific radioactivity (radioactivity/mass labeled and unlabeled DTPA-OC) ranges from 17 to 25 MBq (0.46 to 0.67 mCi) (9).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SDZ%20215-811%22%5BSubstance%20Name%5D%20AND%20%22in%20vitro%22%5BAll%20Fields%5D)]

In vitro studies performed on SSR subtype 2 (sst_2_)-positive rat pancreatic tumor cell lines CA20948 and AR42J and on the SSR-negative human anaplastic thyroid tumor cell line ARO showed that the internalization and the degradation of ^111^In-DTPA-OC were receptor-specific, time- and temperature-dependent processes (11). The receptor-mediated internalization of ^111^In-DTPA-OC results in the degradation to the final radiolabeled metabolite ^111^In-DTPA-D-Phe. This metabolite is unable to pass through the lysosomal or other cell membrane(s) because of its polarity and, therefore, stays in the lysosomes, causing the long intracellular retention time of ^111^In in sst_2_-positive tumor cells.

The therapeutic effect of ^111^In-DTPA-OC has been shown in several in vitro studies, such as the one by Duncan et al. (12) on sst_2_-positive rat pancreatic tumor cell line CA20948.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SDZ%20215-811%22%5BSubstance%20Name%5D%20AND%20%22rodentia%22%5BMeSH%5D)]

Only a limited number of animal models using human tumor tissue have been developed for experimental studies of radiolabeled OC. This is because human NE tumor cell lines expressing SSRs are uncommon. Pharmacokinetic and therapeutic studies have been performed essentially using rat exocrine pancreatic tumors (13, 14). A study by Adrian et al. (15) on nude mice carrying the human carcionoid GOT1 showed that the uptake in tumor and normal organs varied with the amount and administration mode of ^111^In-DTPA-OC. Uptake was highest in tumor after 0.1 and 1 µg of ^111^In-DTPA-OC and lowest in muscle, heart, and blood after 0.1 µg. The uptake decreased in lungs and spleen with higher amounts of ^111^In-DTPA-OC, and in all organs studied, the tumor/normal tissue activity concentration ratio was maximal at 0.1 and 1 µg.

In separate in vivo studies on rats, Breeman et al. (16) and Kwekkeboom et al. (17) showed that the uptake of ^111^In-DTPA-OC in receptor-positive tissues was not maximal at the lowest possible peptide amount or maximum-specific activity but was a bell-shaped function of the injected mass. Experimental data from rat studies by Slooter et al. (18) showed that high doses of ^111^In-DTPA-OC could inhibit the growth of liver metastases after injection of sst_2_ receptor-positive tumor cells in the portal vein, and that the number of SSR-positive liver metastases was significantly decreased after treatment with ^111^In-DTPA-OC.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22 SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

^111^In-DTPA-OC scintigraphy was used to localize and stage spontaneously occurring insulinomas and gastrinomas in dogs (19, 20). In a study by Robben et al. (20), primary tumors and/or metastases of <3 mm in dogs could be visualized and localized by single photon emission computed tomography (SPECT) imaging. In vitro autoradiography and ligand binding studies showed that canine insulinomas expressed one subtype of SSR (sst_2_). This is in contrast with findings in humans where, on the basis of ligand binding studies, different subtypes of SSRs have been identified.

SPECT imaging studies showed that in dogs, abdominal organ accumulation of ^111^In-DTPA-OC primarily occurred in the kidneys, liver, gallbladder, gastric fundus, and intestines. This is very similar to what was reported in humans, except for the stomach, which shows no accumulation in human studies. Dog studies showed no splenic accumulation, and ^111^In-DTPA-OC was primarily excreted via the kidneys (20, 21).

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SDZ%20215-811%22%5BSubstance%20Name%5D%20AND%20%28%28%28%22primates%22%5BTIAB%5D%20NOT%20Medline%5BSB%5D%29%20OR%20%22primates%22%5BMeSH%20Terms%5D%20OR%20primate%5BText)]

No reference currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SDZ%20215-811%22%5BSubstance%20Name%5D%20AND%20%28%28%22humans%22%5BTIAB%5D%20NOT%20Medline%5BSB%5D%29%20OR%20%22humans%22%5BMeSH%20Terms%5D%20OR%20human%5BText%20Word%255)]

In vivo human studies showed that ^111^In-DTPA-OC was distributed to and localized in tumors within about 1 h of intravenous administration, and it was retained in the normal pituitary and thyroid glands, liver, spleen, urinary bladder, and to a lesser extent, in the bowel (22, 23). Hepatic and biliary accumulations were found to be 2% of the administrated activity 4 h after injection. Organs showing the maximal retention were the spleen and kidneys, with estimated absorbed radiation doses of about 0.66 mGy/MBq (2.46 rad/mCi) and 0.49 mGy/MBq (1.80 rad/mCi), respectively. However, these estimated doses were found to be lower in the liver, spleen, and kidney, with patients bearing large tumors positive for SSRs (15).

The effective dose of ^111^In-DTPA-OC for humans, based on data from the International Commission on radiological protection (ICRP) Publication 53 and reported in the OctreoScan kit, is 0.12 mSv/MBq (0.43 rem/mCi). Krenning et al. (21) reported a calculated effective dose equivalent of 0.08 mSv/MBq. Kwekkeboom et al. (17) reported a preferred dose of about 200 MBq (5.40 mCi), which makes it possible to perform SPECT and gives a better anatomic delineation than planar views.

It was shown that when a standard dose of 220 MBq (5.95 mCi) ^111^In was coupled to <5 µg of DTPA-OC, the quality of scintigraphy was decreased, and the uptake in tumors was significantly reduced. ^111^In-DTPA-OC scans should always be performed with at least 10 µg of peptide (as supplied in the OctreoScan kit formulation) (6).

Because of its relatively long effective half-life, ^111^In-DTPA-OC may be used to see SSR-bearing tumors efficiently after 24 and 48 h, when interfering background radioactivity is minimized by renal clearance. Planar and SPECT studies should be performed preferably 24 h after injection. A higher lesion-detection rate of 24-h planar imaging over 4-h acquisition was reported by Jamar et al. (24).

Biodistribution studies by Forssell-Aronsson et al. (25) on tumors (breast and medullary thyroid carcinoma (MTC), differentiated thyroid tumors, endocrine pancreatic tumors (EPTs)) and normal tissues showed large inter- and intra-individual variations in ^111^In activity concentration. This concentration was, in general, higher in carcinoids and some EPTs (range, 0.33-77% injected dose (ID)/kg) than in MTC and other tumors (0.017-7.8% ID/kg). Tumor/blood ratios >100 were found in most patients with carcinoids, EPTs, renal carcinoma, and neuroendocrine carcinoma (maximum value, 1500), whereas tumor/blood ratios were >80 in most other tumors. Normal tissue/blood ratios were in general ≤10, but higher values were found in liver, kidneys, and spleen.

Over recent years, various human studies aimed at investigating the potential ^111^In-DTPA-OC in radionuclide therapy have been performed and reported in the literature (17, 26, 27).

## References

1 Kubota A, et al. (1994). Identification of somatostatin receptor subtypes and an implication for the efficacy of somatostatin analogue SMS 201-995 in treatment of human endocrine tumors. J Clin Invest.
2 Yamada Y, et al. (1992). Cloning and functional characterization of a family of human and mouse somatostatin receptors expressed in brain, gastrointestinal tract, and kidney. Proc Natl Acad Sci U S A.
3 Slooter GD, et al. (2001). Somatostatin receptor imaging, therapy and new strategies in patients with neuroendocrine tumours. Br J Surg.
4 Ginj M, et al. (2005). Preclinical Evaluation of New and Highly Potent Analogues of Octreotide for Predictive Imaging and Targeted Radiotherapy. Clin Cancer Res.
5 De Jong M, et al. (2002). Somatostatin receptor-targeted radionuclide therapy of tumors: preclinical and clinical findings. Semin Nucl Med.
6 Valkema R, et al. (2002). Phase I study of peptide receptor radionuclide therapy with [In-DTPA]octreotide: the Rotterdam experience. Semin Nucl Med.
7 Capello A, et al. (2003). Peptide receptor radionuclide therapy in vitro using [111In-DTPA0]octreotide. J Nucl Med.
8 Forster GJ, et al. (2001). Preliminary data on biodistribution and dosimetry for therapy planning of somatostatin receptor positive tumours: comparison of (86)Y-DOTATOC and (111)In-DTPA-octreotide. Eur J Nucl Med.
9 Bakker WH, et al. (1991). [111In-DTPA-D-Phe1]-octreotide, a potential radiopharmaceutical for imaging of somatostatin receptor-positive tumors: synthesis, radiolabeling and in vitro validation. Life Sci.
10 Hnatowich DJ, et al. (1983). Radioactive labeling of antibody: a simple and efficient method. Science.
11 De Jong M, et al. (1998). Internalization of radiolabelled [DTPA0]octreotide and [DOTA0,Tyr3]octreotide: peptides for somatostatin receptor-targeted scintigraphy and radionuclide therapy. Nucl Med Commun.
12 Duncan JR, et al. (1997). Indium-111-diethylenetriaminepentaacetic acid-octreotide is delivered in vivo to pancreatic, tumor cell, renal, and hepatocyte lysosomes. Cancer Res.
13 Froidevaux S, et al. (2000). Preclinical comparison in AR4-2J tumor-bearing mice of four radiolabeled 1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid-somatostatin analogs for tumor diagnosis and internal radiotherapy. Endocrinology.
14 de Jong M, et al. (1999). Tumour uptake of the radiolabelled somatostatin analogue [DOTA0, TYR3]octreotide is dependent on the peptide amount. Eur J Nucl Med.
15 Adrian HJ, et al. (1993). Biodistribution of 111In-pentetreotide and dosimetric considerations with respect to somatostatin receptor expressing tumor burden. Horm Metab Res Suppl.
16 Breeman WA, et al. (1995). Effect of dose and specific activity on tissue distribution of indium-111-pentetreotide in rats. J Nucl Med.
17 Kwekkeboom D, Krenning EP, de Jong M. (2000). Peptide receptor imaging and therapy. J Nucl Med.
18 Slooter GD, et al. (1999). Anti-proliferative effect of radiolabelled octreotide in a metastases model in rat liver. Int J Cancer.
19 Altschul M, et al. (1997). Evaluation of somatostatin analogues for the detection and treatment of gastrinoma in a dog. J Small Anim Pract.
20 Robben JH, et al. (1997). In vitro and in vivo detection of functional somatostatin receptors in canine insulinomas. J Nucl Med.
21 Krenning EP, et al. (1992). Somatostatin receptor scintigraphy with indium-111-DTPA-D-Phe-1-octreotide in man: metabolism, dosimetry and comparison with iodine-123-Tyr-3-octreotide. J Nucl Med.
22 Fischman AJ, Babich JW, Strauss HW. (1993). A ticket to ride: peptide radiopharmaceuticals. J Nucl Med.
23 Krenning EP, et al. (1993). Somatostatin receptor scintigraphy with [111In-DTPA-D-Phe1]- and [123I-Tyr3]-octreotide: the Rotterdam experience with more than 1000 patients. Eur J Nucl Med.
24 Jamar F, et al. (1995). Somatostatin receptor imaging with indium-111-pentetreotide in gastroenteropancreatic neuroendocrine tumors: safety, efficacy and impact on patient management. J Nucl Med.
25 Forssell-Aronsson E, et al. (2004). Biodistribution data from 100 patients i.v. injected with 111In-DTPA-D-Phe1-octreotide. Acta Oncol.
26 Pasieka JL, McEwan AJ, Rorstad O. (2004). The palliative role of 131I-MIBG and 111In-octreotide therapy in patients with metastatic progressive neuroendocrine neoplasms. Surgery.
27 McCarthy KE, et al. (1998). In situ radiotherapy with 111In-pentetreotide: initial observations and future directions. Cancer J Sci Am.